# ^64^Cu-Labeled 2,6-bis(dimethylamino)-10-(4-((4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclodo-decan-1-yl)methyl)benzyl)-acridin-10-ium

Chemical name: | ^64^Cu-Labeled 2,6-bis(dimethylamino)-10-(4-((4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclodo-decan-1-yl)methyl)benzyl)-acridin-10-ium
Abbreviated name: | [^64^Cu]DO3A-xy-ACR
Synonym:
Agent Category: | Compound
Target: | Mitochondria; nucleic acids
Target Category: | Other (cell organelle); nucleic acids
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%22acridine%20orange%22%5bMeSH%20Terms%5d%20OR%20%28%22acridine%22%5bAll%20Fields%5d%20AND%20%22orange%22%5bAll%20Fields%5d%29%20OR%20%22acridine%20orange%22%5bAll%20Fields%5d&cmd=DetailsSearch)]

Compared with normal cells, cancer cells have an increased number of mitochondria, and these organelles exhibit an altered metabolism to meet the high nutritional and energy demands required for the survival and uncontrolled proliferation of the cancerous cells. The high metabolic rate of mitochondria results in the production of reactive oxygen species that are believed to assist in the transformation of the surrounding normal cells to the neoplastic phenotype (1). Changes in the bioenergetics of these organelles increases the negative mitochondrial potential (compared with mitochondria in normal cells), which can be measured with cationic organic dyes, such as rhodamine B (a fluorescent dye) and its derivatives, because they tend to accumulate in the mitochondria (2). Therefore, several types of fluorescent tracers have been used with optical imaging techniques and have been shown to be suitable for the visualization of tumors (3, 4). In addition, ^11^C-labeled (t_1/2_ = 20.4 min) or ^18^F-labeled (t_1/2_ = 110 min) lipophilic phosphonium cation derivatives, which are rapidly taken up by mitochondria, have been used in preclinical studies to detect tumors with positron emission tomography (PET) (5) and as myocardial perfusion imaging agents (6). In another study, the biodistribution of [^11^C]rhodamine-123 was investigated in mice, and it was concluded that this tracer is not suitable to measure levels of the P-glycoprotein transporter (P-gp; rhodamine dyes are known to target this transporter in the cells) (7). In addition, the short half-life and the generation of high background signals by this radionuclide in the normal organs of animals limit its application in the clinic (2).

In a continuing effort to develop a radiolabeled probe that can target and accumulate in cellular mitochondria, it has been shown that ^64^Cu-labeled derivatives of rhodamine are suitable for the visualization of cancerous tumors in mice (2). The main advantage of using ^64^Cu over ^11^C or ^18^F to label the rhodamine derivatives is that the former radionuclide is commercially available for use by institutions that lack an on-site cyclotron, which is required to produce ^64^Cu; in addition, this radionuclide has a longer half-life (t_1/2_ = 12.7 h) and high specific activity compared with either ^11^C or ^18^F (2). In another study, using cultured cell–based assays, it was shown that ^99m^Tc-labeled acridines (chemiluminescent compounds that are known to intercalate into duplex DNA) can penetrate the cell nucleus and bind to duplex and triplex DNA (8). On the basis of this information, ^64^Cu-labeled 2,6-bis(dimethylamino)-10-(4-((4,7,10-tris(carboxymethyl)-1,4,7,10-tetraazacyclodo-decan-1-yl)methyl)benzyl)-acridin-10-ium ([^64^Cu]DO3A-xy-ACR) was synthesized and evaluated with PET for the detection of U87MG cell (http://www.atcc.org/Products/All/HTB-14.aspx) glioma xenograft tumors in athymic mice (9). The U87MG cells have a very low expression of the P-glycoprotein and associated proteins that are known to confer multidrug resistance to mammalian cells (9).

### Related Resource Links

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Acridine+orange&Search=Search) with acridine orange

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DO3A-xy-ACR%20synthesis&cmd=DetailsSearch)]

The synthesis of DO3A-xy-ACR and its labeling with ^64^Cu are described elsewhere (9). The radiochemical purity of [^64^Cu]DO3A-xy-ACR was reported to be >95% without high-performance liquid chromatography purification; the radiochemical yield of the tracer was not reported. The specific activity of [^64^Cu]DO3A-xy-ACR was ~1.85 TBq/mmol (~50 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5DDO3A-xy-ACR%20in%20vitro&cmd=DetailsSearch)]

The log P value of [^64^Cu]DO3A-xy-ACR was −2.0 ± 0.2, indicating that the tracer is hydrophilic (9). [^64^Cu]DO3A-xy-ACR was reported to be stable for >24 h in excess ethylenediamine tetraacetic acid (~1 M in 25 mM phosphate buffer, pH 7.4) (9).

Fluorescence microscopy of U87MG cells stained with Cu-DO3A-xy-ACR (final concentration 20 μM) showed that the stain was present primarily in the cellular mitochondria (9). Human fibroblasts, used as negative controls for this study, showed no mitochondrial staining with Cu-DO3A-xy-ACR. In another experiment, it was shown that Cu-DO3A-xy-ACR (green fluorescence) co-localized with rhodamine (red fluorescence) in the mitochondria of the U87MG cells (rhodamine is known to specifically stain mitochondria) (9). These studies indicated that the Cu-labeled stain is taken up by the mitochondria of only those cells that exhibit a neoplastic phenotype (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5DDO3A-xy-ACR%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]DO3A-xy-ACR was investigated in athymic mice bearing U87MG cell tumors (9). The animals (n = 5 mice/time point) were injected with ~111 KBq (~3 μCi) [^64^Cu]DO3A-xy-ACR through the tail vein, and the rodents were euthanized at time points ranging from 0.5 h postinjection (p.i.) to 24 h p.i. to retrieve the organs of interest. The amount of radioactivity in the various organs, including tumors, was determined as percent of injected dose per gram tissue (% ID/g; Table 1), and the tumor/organ uptake (T/O) ratios were calculated (Table 2). At 0.5 h p.i., maximum radioactivity (31.90 ± 3.98% ID/g) was detected in the liver, and by 24 h p.i. the radioactivity had decreased to 8.18 ± 1.27% ID/g. The kidneys showed a nearly constant level of radioactivity for the duration of the study (~2.50 ± 0.55% ID/g). These observations indicated that the tracer was excreted from the rodent system primarily through the hepatobiliary route. The amount of tracer in the tumors increased from 1.07 ± 0.23% ID/g at 0.5 h p.i. to 3.52 ± 1.72% ID/g at 24 h p.i. All other tissues showed an uptake of <1.0% ID/g at all time points. At 24 h p.i., the tumor/muscle, tumor/blood, tumor/heart, tumor/kidney, and tumor/liver ratios were 12.26 ± 8.60, 8.76 ± 2.03, 3.28 ± 1.85, 1.53 ± 0.83, and 0.44 ± 0.25, respectively.

Nude mice bearing U87MG cell tumors (n = 3 animals) were injected with ~9.25 MBq (~250 μCi) [^64^Cu]DO3A-xy-ACR through the tail vein, and whole-body microPET images of the animals were acquired at time points ranging from 0.5 h p.i. to 24 h p.i (9). The tumors were clearly visible at 0.5 h p.i., and the uptake in the lesions was observed to increase up to 24 h p.i. High accumulation of radioactivity was apparent in the liver at all time points. This indicated that the PET study generated results that were similar to those obtained during the biodistribution study (9).

From these studies, the investigators concluded that [^64^Cu]DO3A-xy-ACR can be used to visualize U87MG cell xenograft tumors in mice (9). However, they caution that [^64^Cu]DO3A-xy-ACR is probably not a good tracer to detect cancerous lesions because the high uptake of label by the liver would mask the visualization of tumors in the surrounding tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5DDO3A-xy-ACR%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5DDO3A-xy-ACR%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5DDO3A-xy-ACR%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by research grant R01 CA115883 from the National Cancer Institute, National Institutes of Health.

## References

1 Wallace D.C. (2012). Mitochondria and cancer. Nat Rev Cancer.
2 Zhou Y., Kim Y.S., Yan X., Jacobson O., Chen X., Liu S. (2011). 64Cu-labeled lissamine rhodamine B: a promising PET radiotracer targeting tumor mitochondria. Mol Pharm.
3 Keereweer S., Hutteman M., Kerrebijn J.D., van de Velde C.J., Vahrmeijer A.L., Lowik C.W. (2012). Translational optical imaging in diagnosis and treatment of cancer. Curr Pharm Biotechnol.
4 Ebert B., Grosenick D. (2013). Optical imaging of breast tumors and of gastrointestinal cancer by laser-induced fluorescence. Recent Results Cancer Res.
5 Min J.J., Biswal S., Deroose C., Gambhir S.S. (2004). Tetraphenylphosphonium as a novel molecular probe for imaging tumors. J Nucl Med.
6 Shoup T.M., Elmaleh D.R., Brownell A.L., Zhu A., Guerrero J.L., Fischman A.J. (2011). Evaluation of (4-[18F]Fluorophenyl)triphenylphosphonium ion. A potential myocardial blood flow agent for PET. Mol Imaging Biol.
7 Bao X., Lu S., Liow J.S., Morse C.L., Anderson K.B., Zoghbi S.S., Innis R.B., Pike V.W. (2012). [(1)(1)C]Rhodamine-123: synthesis and biodistribution in rodents. Nucl Med Biol.
8 Agorastos N., Borsig L., Renard A., Antoni P., Viola G., Spingler B., Kurz P., Alberto R. (2007). Cell-specific and nuclear targeting with [M(CO)(3)](+) (M=(99m)Tc, Re)-based complexes conjugated to acridine orange and bombesin. Chemistry.
9 Zhou Y., Kim Y.S., Shi J., Jacobson O., Chen X., Liu S. (2011). Evaluation of 64Cu-labeled acridinium cation: a PET radiotracer targeting tumor mitochondria. Bioconjug Chem.

Table 1: Uptake of radioactivity from [^64^Cu]DO3A-xy-ACR in various tissues of athymic mice bearing U87MG cell tumors at different time points.

Tissues | Accumulated radioactivity (% ID/g) at different time points p.i.
Tissues | 0.5 h | 1 h | 2 h | 4 h | 24 h
Blood | 0.90 ± 0.22 | 0.60 ± 0.17 | 0.70 ± 0.08 | 0.70 ± 0.19 | 0.53 ± 0.05
Heart | 0.66 ± 0.25 | 0.66 ± 0.08 | 0.70 ± 0.11 | 0.89 ± 0.13 | 1.14 ± 0.33
Kidney | 2.89 ± 0.90 | 2.53 ± 0.37 | 2.63 ± 0.42 | 2.18 ± 0.39 | 2.38 ± 0.41
Liver | 31.90 ± 3.98 | 24.95 ± 5.64 | 15.20 ± 4.29 | 14.09 ± 6.82 | 8.18 ± 1.27
Muscle | 0.29 ± 0.18 | 0.24 ± 0.11 | 0.20 ± 0.13 | 0.33 ± 0.06 | 0.34 ± 0.17
Tumor | 1.07 ± 0.23 | 1.58 ± 0.55 | 2.71 ± 0.66 | 3.47 ± 1.19 | 3.52 ± 1.72

For complete data, see Zhou et al. (9).

Table 2: Tumor/organ tracer uptake ratios at various time points in athymic mice bearing U87MG glioma cell lesions.

Organ | Uptake ratios at different time points p.i.
Organ | 0.5 h | 1 h | 2 h | 4 h | 24 h
Blood | 1.23 ± 0.29 | 2.82 ± 1.04 | 3.96 ± 1.29 | 5.40 ± 3.66 | 8.76 ± 2.03
Heart | 1.79 ± 0.60 | 2.46 ± 0.98 | 3.99 ± 1.28 | 3.94 ± 2.17 | 3.28 ± 1.85
Kidney | 0.41 ± 0.16 | 0.61 ± 0.16 | 1.05 ± 0.29 | 1.63 ± 0.92 | 1.53 ± 0.83
Liver | 0.03 ± 0.01 | 0.07 ± 0.02 | 0.20 ± 0.09 | 0.31 ± 0.25 | 0.44 ± 0.25
Lung | 0.66 ± 0.10 | 0.97 ± 0.23 | 1.55 ± 0.26 | 1.89 ± 0.70 | 1.92 ± 0.87
Muscle | 4.90 ± 2.56 | 7.52 ± 3.91 | 17.82 ± 8.66 | 11.54 ± 8.06 | 12.26 ± 8.60

For complete data, see Zhou et al. (9).